# 5-[(E)-2-(4-[^18^F]Fluorophenyl)ethenyl]-1,3-benzenediol

Chemical name: | 5-[(E)-2-(4-[^18^F]Fluorophenyl)ethenyl]-1,3-benzenediol
Abbreviated name:
Synonym: | 3,5-Dihydroxy-4'-[^18^F]fluoro-trans-stilbene
Agent Category: | Compound
Target: | Potential targets: nuclear factor κB (NF-κB); activator protein 1 (AP-1)
Target Category: | Binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20AND%20resveratrol)]

Resveratrol, a polyphenolic phytoalexine and a derivative of stilbene, is produced in plants via an enzymatic reaction with stilbene synthase. It exists in two isomeric forms: cis- (Z) and trans- (E), trans- being the most abundant and biologically active form.

Over the past decade, resveratrol has been shown to be effective against neuronal cell dysfunction and cell death (1), offering some protection against atherosclerosis (including the inhibition of low-density lipoprotein) (2). Resveratrol was also shown to have cancer chemopreventive activity in all three stages of carcinogenesis (3, 4). Resveratrol was reported to prevent tumor growth and metastasis in human lung carcinoma, in pancreatic and prostate cancer, and in bronchial epithelioma cancer models. Resveratrol may also be useful in Huntington’s disease and Alzheimer’s disease (5).

Despite the very favorable research results reported in the literature, the bioavailability and metabolic pathways of resveratrol in vivo are still uncertain. The initial phases in the cellular action of resveratrol (as an antitumor agent) have not been fully understood, and a cellular receptor site where the signal is initiated has not been described. Several research studies have reported that resveratrol has the ability to induce p53-dependent apoptosis in several cancer cell lines, and that the signal transduction pathways implicated in resveratrol action includes those of extracellular-regulated kinases 1 and 2 (ERK1/2), p38 kinase, and Jun N-terminal kinase (JNK) (6, 7). Lin et al (8). showed that the binding of resveratrol to integrin αVß3, principally to the ß3 monomer, was essential for transduction of the stilbene signal into p53-dependent apoptosis of breast cancer cells.

With respect to imaging, outstanding issues include the major drawbacks of ^14^C-labeled compounds that have been used so far to investigate the mechanisms involved in the pharmacologic activity of resveratrol (e.g., difficulty in obtaining total recovery from the subject, kinetic measurements causing experimental expenditure with β^-^ nuclides). ^11^C or ^18^F used with positron emission tomography (PET) represent better alternatives, and several studies are currently underway. The first results using PET and the resveratrol derivative 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene in rodents were reported by Gester et al. (9) in 2005.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20AND%20resveratrol%20AND%20synthesis)]

The radiosynsthesis of 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene was reported by Gester et al. (9) in 2005. The procedure involved a Homer-Wadsworth-Emmons reaction (three-step/one-pot), and produced 3,5-dihydroxy-4´-[18F]fluoro-trans-stilbene in 120–130 min (HPLC separation included), with a specific activity of ~ 90 GBq/µmol (243 mCi/µmol), a radiochemical yield and purity of ~ 9% (decay-corrected, related to ^18^F-labeled fluoride), and a purity of >97%.

The main steps of the synthesis involved preparing the 4-[^18^F]fluorobenzaldehyde as described by Maeding and Steinbach (10), starting with 4-trimethylammonium-benzaldehyde triflate dissolved in N,N-dimethylmethanamide (DMF) and heated at 120°C for 15 min. After cooling at 60°C, the precursor (diethyl[3,5-bis(methoxymethoxy)benzyl]phosphonate) and KOB were added to the mixture. The coupling-reaction was carried out for 15 min, after which HCl was added to remove the MOM-protecting groups. The mixture was then eluted several times to finally obtain the ^18^F-radiolabeled resveratrol derivative 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20AND%20resveratrol%20AND%20in%20vitro)]

Gester et al. (9) performed in vitro studies to investigate the metabolism of 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene. They observed that after incubation with human hepatocyte (HepG_2_) cells for 30 min, 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene was significantly metabolized, with a major radioactive metabolite present in cell lysates and representing up to 11% and 59% of total ^18^F radioactivity at 4°C and 37°C, respectively. Additional ex vivo and in vivo studies showed that 70% of the total plasma radioactivity could be attributed to two major metabolites ~ 32% and >40% of the total ^18^F radioactivity, see Rodents section for more details).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29resveratrol%20AND%20%28rodentia%5BMeSH%5D%20OR%20rat%29)]

Gester et al. (9) performed the first ex vivo and in vivo radiopharmacological evaluation of 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene using PET. Experiments were carried out with male Wistar rats (6 weeks old; 160–170 g) intravenously injected with single doses of the radiotracer for 15 s [1.5 MBq (0.04 mCi) in 0.5 ml saline with 2% ethanol].

In vivo biodistribution studies showed that 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene was very rapidly cleared from the blood compartment because of the high uptake levels in the liver and kidneys, followed by hepatobiliary and renal elimination. The measured radioactivity concentration (n = 4) at 5 and 60 min after injection represented 28.8 ± 5.1 and 37.9 ± 5.2% of the injected dose (ID), respectively. Respective values at 5 and 60 min after injection for the intestine were 4.8 ± 0.8 and 31.1 ± 3.0% ID, 9.50 ± 0.35 and 5.59 ± 1.23% ID for the kidney, 25.56 ± 3.29 and 12.59 ± 1.11% ID for the liver, 0.58 ± 0.20 and 0.06 ± 0.01% ID for the brain, 2.27 ± 0.32 and 0.49 ± 0.03% ID for the lung, and 0.29 ± 0.03 and 0.08 ± 0.01% ID for the heart. A low accumulation of the ^18^F radioactivity in the femoral bone (0.19 ± 0.02 and 0.05 ± 0.01% ID at 5 and 60 min, respectively) showed that in vivo defluorination of the radiotracer was very limited.

Ex vivo urine samples taken 60 min after injection of the radiotracer showed that > 65% of the total plasma radioactivity could be attributed to two major metabolites, Mb1 and Mb2, representing approximately 32% and > 40% of total ^18^F radioactivity. For samples taken from the intestines, those values were approximately 47% and 26% for Mb1 and Mb2, respectively. Taking into consideration the data obtained from their studies and other published research results (11-13), Gester et al (9). suggested that Mb1 was probably a glucuronide and Mb2 was a sulfate of 3,5-dihydroxy-4´-[^18^F]fluoro-trans-stilbene. However, additional studies are needed to clearly identify the metabolites involved.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29resveratrol%20AND%20%28dog%20OR%20sheep%20OR%20pig%20OR%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29resveratrol%20AND%20humans%5BMeSH%5D)]

No publication is currently available.

## References

1 Michels G, Watjen W, Weber N, Niering P, Chovolou Y, Kampkotter A, Proksch P, Kahl R. (2006). Resveratrol induces apoptotic cell death in rat H4IIE hepatoma cells but necrosis in C6 glioma cells. Toxicology.
2 Norata GD, Marchesi P, Passamonti S, Pirillo A, Violi F, Catapano AL. (2006). . Anti-inflammatory and anti-atherogenic effects of cathechin, caffeic acid and trans-resveratrol in apolipoprotein E deficient mice. Atherosclerosis.
3 Kundu JK, Surh YJ. (2004). Molecular basis of chemoprevention by resveratrol: NF-kappaB and AP-1 as potential targets. Mutat Res.
4 Delmas D, Lancon A, Colin D, Jannin B, Latruffe N. (2006). Resveratrol as a chemopreventive agent: a promising molecule for fighting cancer. Curr Drug Targets.
5 Marambaud P, Zhao H, Davies P. (2005). Resveratrol promotes clearance of Alzheimer's disease amyloid-beta peptides. J Biol Chem.
6 She QB, Huang C, Zhang Y, Dong Z. (2002). Involvement of c-jun NH(2)-terminal kinases in resveratrol-induced activation of p53 and apoptosis. Mol Carcinog.
7 Shih A, Zhang S, Cao HJ, Boswell S, Wu YH, Tang HY, Lennartz MR, Davis FB, Davis PJ, Lin HY. (2004). Inhibitory effect of epidermal growth factor on resveratrol-induced apoptosis in prostate cancer cells is mediated by protein kinase C-alpha. Mol Cancer Ther.
8 Lin HY, Lansing L, Merillon JM, Davis FB, Tang HY, Shih A, Vitrac X, Krisa S, Keating T, Cao HJ, Bergh J, Quackenbush S, Davis PJ. (2006). Integrin alphaVbeta3 contains a receptor site for resveratrol. FASEB J.
9 Gester S, Wuest F, Pawelke B, Bergmann R, Pietzsch J. (2005). Synthesis and biodistribution of an 18F-labelled resveratrol derivative for small animal positron emission tomography. Amino Acids.
10 Maeding P, Steinbach J. (2002). Synthesis of 4-[18F]fluorobenzaldehyde - an important labelling moiety in F18 chemistry. Institute of Bioinorganic and Radiopharmaceutical Chemistry: Annual Report 2001 : p. 58.
11 Walle T, Hsieh F, DeLegge MH, Oatis JE, Walle UK. (2004). High absorption but very low bioavailability of oral resveratrol in humans. Drug Metab Dispos.
12 Walle T. (2004). Absorption and metabolism of flavonoids. Free Radic Biol Med.
13 Kuhnle G, Spencer JP, Chowrimootoo G, Schroeter H, Debnam ES, Srai SK, Rice-Evans C, Hahn U. (2000). Resveratrol is absorbed in the small intestine as resveratrol glucuronide. Biochem Biophys Res Commun.